# ^11^C-Labeled rifampicin

Chemical name: | ^11^C-Labeled rifampicin | [image]
Abbreviated name: | [^11^C]RIF | [image]
Synonym: | ^11^C-Labeled rifampin | [image]
Agent Category: | Compounds | [image]
Target: | DNA-dependent RNA polymerase in bacterial cells | [image]
Target Category: | Enzymes (bacteria) | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^11^C | [image]
Activation: | No | [image]
Studies: | - In vitro; - Non-human primates | Structure of [^11^C]RIF by Liu et al (1). Click on the PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=tuberculosis+and+rifamycin) for additional information.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=drug+development+and+PET+imaging+and+review)]

Rifampicin (RIF) (or rifampin) is a rifamycin derivative with a clinically effective group of 4-methyl-1-piperazinaminyl. RIF is typically used to treat Mycobacterium infections, including tuberculosis (TB) (1, 2). By binding the β subunit, RIF inhibits the DNA-dependent RNA polymerase and thus prevents RNA and protein synthesis in bacterial cells (2, 3). RIF labeled with ^11^C ([^11^C]RIF) has been generated by Liu et al. for in vivo and real-time analysis of the RIF pharmacokinetics (PK) and biodistribution with positron emission tomography (PET) (1). The half-life of ^11^C is 20.4 min.

The PK and biodistribution of a novel drug are traditionally determined with blood and tissue sampling and/or autoradiography. Despite high workload and huge investment in drug development, only 8% of the drugs entering clinical trials today reach the market as estimated by the U.S. Food and Drug Administration (http://www.fda.gov/ScienceResearch/SpecialTopics/CriticalPathInitiative/CriticalPathOpportunitiesReports/ucm077262.htm). One main reason for this attrition is insufficient exploration of the in vivo drug-target interaction (1). Traditional methods are inadequate to answer questions such as whether a drug reaches the target, how the drug interacts with its targets, and how the drug modifies the diseases. Because of the high resolution and sensitivity of newly developed imaging techniques, investigators have become increasingly interested in addressing these issues (4, 5). In the case of PET imaging, most small molecules can now be efficiently labeled with ^11^C or with ^18^F at >37 GBq/µmol (1 Ci/μmol), and they can be detected with PET in the nanomolar to picomolar concentration range (6-8). Consequently, a sufficient signal for imaging can be obtained even though the total amount of a radiotracer administered systemically is extremely low (known as microdosing, typically <1 μg for humans). Microdosing is particularly valuable for evaluating tissue exposure in the early phase of drug development when the full-range toxicology is not yet available (9, 10). Increasing evidence has demonstrated the efficiency of PET imaging in: obtaining quantitative information on drug PK and distribution in various tissues including brain; confirming drug binding with targets and elucidating the relationship between occupancy and target expression/function in vivo; assessing drug passage across the blood–brain barrier (BBB) and ensuring sufficient exposure to brain for central nervous system drugs; and dissecting the modifying effects of drugs on diseases (4, 6, 7).

The current treatment regime for drug-sensitive TB involves the use of RIF, isoniazid (INH), pyrazinamide (PZA), and ethambutol or streptomycin for two months, followed by four months of continued dosing with INH and RIF (2, 3). This regime is primarily based on PK studies in serum and efficacy of treatment. The efficacy of each drug for different types of TB such as brain TB and the drug distribution in each compartment of an organ are not well understood. To provide direct insights into these drugs, Liu et al. labeled INH, RIF, and PZA with ^11^C and investigated their PK and biodistribution in baboons with PET (1). Liu et al. found that the organ distribution and BBB penetration of each drug differed greatly. For [^11^C]RIF, its ability to penetrate the BBB was lower than that of PZA and INH (PZA > INH). The RIF concentrations in the lungs and brain were 10 times and 3−4 times higher, respectively, than the RIF minimum inhibitory concentration (MIC) value against TB, supporting the use of RIF for treating TB infections in the lungs and the central nervous system. This chapter summarizes the data of [^11^C]RIF obtained by Liu et al. The data obtained with [^11^C]INH and [^11^C]PZA were described in the MICAD chapters on [^11^C]INH and [^11^C]PZA, respectively.

### Related Resource Links:

- Challenge and Opportunity on the Critical Path to New Medical Products, FDA (http://www.fda.gov/ScienceResearch/SpecialTopics/CriticalPathInitiative/default.htm)
- Rifamycin derivatives in PubChem Substance (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=tuberculosis+and+rifamycin)
- Clinical trials for diagnosis and treatment of tuberculosis in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=tuberculosis)
- MICAD chapters on [^11^C]INH and [^11^C]PZA (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20205479)]

Liu et al. first synthesized the demethyl RIF (RIF precursor) and generated the [^11^C]CH_3_I from [^11^C]CO_2_ (1). Radiolabeling of the RIF piperazine moiety with [^11^C]CH_3_I was then accomplished with potassium carbonate and the combination of dimethyl sulfoxide and MeCN. The labeled product was subsequently purified, and ascorbic acid was added to prevent oxidation. The average decay-corrected yield of [^11^C]RIF, calculated from [^11^C]CH_3_I, was 15−25% with a total synthesis time of 50 min. [^11^C]RIF was >99% radiochemically pure with a specific activity of 21.46 GBq/µmol (580 mCi/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20205479)]

The lipophilicity (logD) of [^11^C]RIF was measured on the basis of octanol−water partitioning. The plasma protein binding (% of free fraction in plasma) of [^11^C]RIF was determined after incubation with baboon plasma for 10 min at room temperature. The logD was 1.67 and the plasma protein binding was 27.32%, which are similar to literature values reported elsewhere (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20205479)]

Liu et al. studied the biodistribution of [^11^C]RIF in healthy baboons (n = 4) with PET imaging (1). The RIF concentrations in the brain and other organs were estimated on the basis of the weight of the baboon (17 kg), a standard drug dose (20 mg/kg), and the assumption that the positron signal derives primarily from the intact drug. Studies showed that the penetrating ability of [^11^C]RIF and/or its radiolabeled metabolites through the BBB was weaker than that of PZA and INH. The RIF concentration in the brain tissue was higher than in the cerebrospinal fluid. The concentration in the whole brain was 0.000642% injected dose per cubic centimeter (ID/cc) (1.09 μg/ml) at 30 min, 0.000536% ID/cc (0.912 μg/ml) at 60 min, and 0.000710% ID/cc (1.21 μg/ml) at 90 min after injection, which was three to four times higher than its MIC against TB. The detailed data about the [^11^C]RIF distribution in other organs were presented in table 2 in the paper published by Liu et al. In general, [^11^C]RIF showed a moderate distribution in the heart, lungs, and kidneys, and was then concentrated in the liver and gallbladder. In most organs, the RIF concentration exceeded that observed in plasma over the 90-min period except for the cortex of kidney at 60 min. The RIF concentration in the lungs was >10 times higher than its MIC. Liu et al. concluded that the RIF concentrations determined by imaging the distribution of [^11^C]RIF in healthy baboons were similar to those observed previously in mice, monkeys, and human, while PET imaging provided dynamic data from 0 min to 90 min. The PET imaging results supported the use of RIF for treating TB infections in the lungs and brain (1).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Liu L., Xu Y., Shea C., Fowler J.S., Hooker J.M., Tonge P.J. (2010). Radiosynthesis and bioimaging of the tuberculosis chemotherapeutics isoniazid, rifampicin and pyrazinamide in baboons. J Med Chem.
2 Aristoff P.A., Garcia G.A., Kirchhoff P.D., Hollis Showalter H.D. (2010). Rifamycins--obstacles and opportunities. Tuberculosis (Edinb).
3 Tomioka H. (2006). Current status of some antituberculosis drugs and the development of new antituberculous agents with special reference to their in vitro and in vivo antimicrobial activities. Curr Pharm Des.
4 Fox G.B., Chin C.L., Luo F., Day M., Cox B.F. (2009). Translational neuroimaging of the CNS: novel pathways to drug development. Mol Interv.
5 Komoda F., Suzuki A., Yanagisawa K., Inoue T. (2009). Bibliometric study of radiation application on microdose useful for new drug development. Ann Nucl Med.
6 Hammond L.A., Denis L., Salman U., Jerabek P., Thomas C.R., Kuhn J.G. (2003). Positron emission tomography (PET): expanding the horizons of oncology drug development. Invest New Drugs.
7 Lancelot, S. and L. Zimmer, Small-animal positron emission tomography as a tool for neuropharmacology. Trends Pharmacol Sci, 2010
8 Lee C.M., Farde L. (2006). Using positron emission tomography to facilitate CNS drug development. Trends Pharmacol Sci.
9 Bauer M., Wagner C.C., Langer O. (2008). Microdosing studies in humans: the role of positron emission tomography. Drugs R D.
10 Wagner C.C., Muller M., Lappin G., Langer O. (2008). Positron emission tomography for use in microdosing studies. Curr Opin Drug Discov Devel.